# [18F]6-fluoro-3-O-methyl-L-3,4-dihydroxyphenylalanine

Chemical name: | [^18^F]6-fluoro-3-O-methyl-L-3,4-dihydroxyphenylalanine
Abbreviated name: | [^18^F]OMFD
Synonym: | 3-O-methyl-6-[^18^F]-fluoro-L-DOPA
Agent Category: | Compound
Target: | L amino acid transporters (LAT)
Target Category: | Binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-Primate Mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+OMFD&WebEnv=0_IrKu54rUXySHgWXB0EaSRAhFOTGAkkCYxv1gd8xknIMbK_U82iUMkAkknBE0o_AKZluhEt3k5W-%407748428072881B60_0000SID&WebEnvRq=1)]

Although ^18^F-fluorodeoxyglucose (^18^F-FDG) is considered the gold standard for the detection of tumors using positron emission tomography (PET), the use of this agent as a tumor diagnostic agent has a limitation (1, 2): the uptake of ^18^F-FDG by cells is based on the glucose transport system. An increased glucose metabolism is a characteristic feature of cancer cells, so this feature can be used to distinguish the neoplastic from normal cells. However, because the uptake of ^18^F-FDG is nonspecific, use of this agent does not distinguish between cells that are cancerous and those that take up ^18^F-FDG because of other etiologies such as inflammation, infection, or even brown fat or granulomas, etc (2). Also, slow-growing malignant tissues (such as prostate tumors) might not show an increased glucose metabolism and thus can not be detected with ^18^F-FDG (3). As a consequence, many other radiolabeled ligands, such as amino acids or their derivatives, have been developed and used for the detection and diagnosis of malignant tumors (1).

In this regard, methionine labeled with radioactive carbon (as ^11^C) has been developed and extensively evaluated for the detection of neoplastic lesions. However, because the label has a short half-life, several ^18^F amino acid analogs have been generated and studied for the diagnosis of neoplastic lesions with PET (4). An increased uptake of amino acids that correlated with upregulation of the amino acid transport system in proliferating cells was observed, and this resulted in a high tumor/normal tissue ratio regardless of the cell cycle phase (4, 5). In the pursuit of developing agents for the detection of cancers, investigators have evaluated a phenylalanine derivative, 3-O-methyl-6-^18^F-fluoro-L-3,4-dihydroxyphenylalanine (^18^F-OMFD), for tumor imaging (6, 7). ^18^F-OMFD was shown to be taken up by neoplastic cells and has been suggested to be suitable for the detection of squamous cell head and neck carcinoma by imaging (8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+OMFD+synthesis&WebEnv=0uIZ3Gd0zYyNO6aIfaLqFjJwLH28OGaztUrAMW8jsoHJ6mfpIiqnmBiikiuWg8JKTy_84FhmmAN63%407748428072881B60_0000SID&WebEnvRq=1)]

The synthesis of ^18^F-OMFD has been detailed by Fϋchtner and Steinbach (9). Briefly, a precursor of ^18^F-OMFD, N-formyl-3-O-methyl-4-O-ditert-butyldicarbonate-6-trimethyl-stannyl-L-dihydroxyphenylalanine-ethyl ester was derived from N-formyl-3,4-O-ditert-butyldicarbonate-6-trimethylstannyl-L-dihydroxyphenylalanine-ethyl ester as described by Namavari et al. (10). The precursor was dissolved in trichlorofluoromethane at room temperature and reacted with gaseous ^18^F-fluorine while the temperature was decreased to -20^o^C. Subsequently, 12 M hydrochloric acid was added to the reaction mixture and the temperature was increased to 70^o^C. Excess solvent was evaporated by blowing gaseous nitrogen through the mixture. The reaction vessel was then closed, and a partial hydrolysis of the products was allowed to proceed at 130^o^C for 10 min at an elevated pressure. Subsequently, ^18^F-OMFD was separated from the reaction mixture by high-performance liquid chromatography on a C-8 column. The total time taken for preparation at the end of bombardment was 50 min with a yield of 20–25% (decay corrected, as related to ^18^F-fluorine). The radiochemical purity of ^18^F-OMFD was >98% with a specific activity of ~20 GBq/mmol (540 mCi/mmol) in ~50 preparations (9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+OMFD+in+vitro&WebEnv=0lA4DTYa3TC5aFjBVEMTlsYyhFH4Dc0tOy9-lBw_NENLlvlw2ECf2HMeDU1C8xd-MeBe4VlLoIggP%407748428072881B60_0000SID&WebEnvRq=1)]

The in vitro uptake of ^18^F-OMFD was investigated in HT-29 (of human colon adenocarcinoma origin), FaDu (of squamous cell carcinoma origin), and RBE4 (of rat brain origin) cell lines in the presence or absence of a competitive transport inhibitor such as 2-aminobicyclo-[2,2,1]-heptane-2-carboxylic acid and α-(methylamino)isobutyric acid plus serine and with or without sodium (6). The transport of ^18^F-OMFD was shown to be mediated primarily through a high-capacity, sodium-independent, amino acid transport system, and the FaDu cells showed the highest uptake.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+OMFD+rodentia&WebEnv=0dvWn3ewhFZWU1HbhWtnHtvNQS7B1PVu2_EryGYAz9lN5a0Ve_ftjtXt5fOZRgKgvieY-o7f-Yj3S%407748428072881B60_0000SID&WebEnvRq=1)]

Using PET, Haase et al. investigated the uptake of ^18^F-OMFD in mice bearing FaDu or HT-29 cell xenograft tumors (8). Maximum radioactivity was observed to accumulate in the tumors and the pancreas in both tumor models. The uptake was higher in the FaDu tumors with a standardized uptake value (SUV) of 3.07 ± 0.66 compared to 1.19 ± 0.26 for the HT-29 cell tumors. From this study the investigators concluded that ^18^F-OMFD could be used for the detection of poorly differentiated, squamous cell tumors in the head and neck (8).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+OMFD+non+primate+mammals&WebEnv=0FWwJlATp07WBPnZDUa5ON7Gh1kdyb-4TVYQjhqG3PaL39q_FpsXfCCiAD9fnFfHRRBHVx7eEcpqp%407748428072881B60_0000SID&WebEnvRq=1)]

The transport of ^18^F-OMFD and ^18^F-dihydroxyphenylalanine (^18^F-DOPA) across the blood–brain barrier (BBB) was investigated with PET in pigs of different ages (11). The transport rate of both neutral amino acids across the BBB was observed to decrease as the brains of the animals developed, but the cerebral blood flow and the plasma concentrations of these amino acids did not change during brain development. The transport of ^18^F-OMFD and ^18^F-DOPA was mediated primarily by the L amino acid transporter 1. Data from the study indicated that developmental changes of the transporter system for neutral amino acids in these animals after birth lead to a decrease in the BBB permeability for these amino acids during brain development.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+OMFD+non+human+primates&WebEnv=02RYvRAUdltz082zFscEWZdz49hVAdPERQ8TmJfcU6iiVt8SBMeDDutWyR5Bs_b342rOVdp4dcZnG%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+OMFD+human+&WebEnv=01FbSaIJHyDmI9fvs3VPMYDjRGZsXh6b0wLFze2oG2AVyRMhCbJeqf8eOmazsRHIFlu9Ba99MsE3Q%407748428072881B60_0000SID&WebEnvRq=1)]

The use of ^18^F-OMFD for brain tumor imaging and whole-body biodistribution was studied using PET in humans (7). With this technique, 16 of 19 studied patients were suspected to have viable brain tumors with a standardized uptake value of 3.0 ± 0.8 and a tumor/non-tumor ratio of 1.9 ± 0.5. Maximum uptake of the label was observed between 15 and 30 min after administration with a subsequent slow decrease in uptake. The label did not accumulate in any specific organ and was eliminated through the urinary system (7). The investigators caution that, although ^18^F-OMFD appears to be a suitable agent to image brain tumors, because it has been evaluated in only a small number of patients it remains to be demonstrated that it is as specific as O-(2-[^18^F]fluoroethyl)-L-tyrosine to differentiate between a tumor and inflammation or as promising as 3-[^18^F]fluoro-L-α-methyl-tyrosine to image malignant tumors (7).

In another study, the use of ^18^F-OMFD was compared to that of ^18^F-FDG and ^18^F-DOPA for the diagnosis of metastatic medullary thyroid carcinoma (MTC) (12). With results from this study the investigators concluded that, although ^18^F-FDG and ^18^F-DOPA could detect highly suspicious foci, suggesting local recurrence or metastasis of MTC, the foci were not detected with ^18^F-OMFD.

## Supplemental Information

[Disclaimers]

## References

1 Chen W. (2007). Clinical applications of PET in brain tumors. J Nucl Med.
2 Groves A.M., Win T., Haim S.B., Ell P.J. (2007). Non-[18F]FDG PET in clinical oncology. Lancet Oncol.
3 Kayani I., Groves A.M. (2006). 18F-fluorodeoxyglucose PET/CT in cancer imaging. Clin Med.
4 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
5 Sasajima T., Miyagawa T., Oku T., Gelovani J.G., Finn R., Blasberg R. (2004). Proliferation-dependent changes in amino acid transport and glucose metabolism in glioma cell lines. Eur J Nucl Med Mol Imaging.
6 Bergmann R., Pietzsch J., Fuechtner F., Pawelke B., Beuthien-Baumann B., Johannsen B., Kotzerke J. (2004). 3-O-methyl-6-18F-fluoro-L-dopa, a new tumor imaging agent: investigation of transport mechanism in vitro. J Nucl Med.
7 Beuthien-Baumann B., Bredow J., Burchert W., Fuchtner F., Bergmann R., Alheit H.D., Reiss G., Hliscs R., Steinmeier R., Franke W.G., Johannsen B., Kotzerke J. (2003). 3-O-methyl-6-[18F]fluoro-L-DOPA and its evaluation in brain tumour imaging. Eur J Nucl Med Mol Imaging.
8 Haase C., Bergmann R., Fuechtner F., Hoepping A., Pietzsch J. (2007). L-Type Amino Acid Transporters LAT1 and LAT4 in Cancer: Uptake of 3-O-Methyl-6- 18F-Fluoro-L-Dopa in Human Adenocarcinoma and Squamous Cell Carcinoma In Vitro and In Vivo. J Nucl Med.
9 Fuchtner F., Steinbach J. (2003). Efficient synthesis of the 18F-labelled 3-O-methyl-6-[18F]fluoro-L-DOPA. Appl Radiat Isot.
10 Namavari M., Bishop A., Satyamurthy N., Bida G., Barrio J.R. (1992). Regioselective radiofluorodestannylation with [18F]F2 and [18F]CH3COOF: a high yield synthesis of 6-[18F]Fluoro-L-dopa. Int J Rad Appl Instrum [A].
11 Brust P., Vorwieger G., Walter B., Fuchtner F., Stark H., Kuwabara H., Herzau M., Opfermann T., Steinbach J., Ganapathy V., Bauer R. (2004). The influx of neutral amino acids into the porcine brain during development: a positron emission tomography study. Brain Res Dev Brain Res.
12 Beuthien-Baumann B., Strumpf A., Zessin J., Bredow J., Kotzerke J. (2007). Diagnostic impact of PET with 18F-FDG, 18F-DOPA and 3-O-methyl-6-[18F]fluoro-DOPA in recurrent or metastatic medullary thyroid carcinoma. Eur J Nucl Med Mol Imaging.